# ^99m^Tc-Bis-amino-bis-thiol-conjugated 6-(3-bromopropoxy)-2-(4-(dimethylamino)phenyl)-4H-chromen-4-one and (Z)-5-(3-bromopropoxy)-2-(4-(dimethylamino)benzylidene)benzofuran-3(2H)-one

Chemical name: | ^99m^Tc-Bis-amino-bis-thiol-conjugated 6-(3-bromopropoxy)-2-(4-(dimethylamino)phenyl)-4H-chromen-4-one and (Z)-5-(3-bromopropoxy)-2-(4-(dimethylamino)benzylidene)benzofuran-3(2H)-one | [image]
Abbreviated name: | [^99m^Tc]BAT-FL, [^99m^Tc]BAT-AR | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | β-amyloid (Aβ) | [image]
Target Category: | Accepters | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR by Ono et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular%20imaging%20and%20Alzheimer%u2019s%20disease%20and%20%u03B2-amyloid%20)]

^99m^Tc-Bis-amino-bis-thiol (BAT)-conjugated 6-(3-bromopropoxy)-2-(4-(dimethylamino)phenyl)-4H-chromen-4-one and (Z)-5-(3-bromopropoxy)-2-(4-(dimethylamino)benzylidene)benzofuran-3(2H)-one, abbreviated as [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR, respectively, are flavone and aurone derivatives synthesized by Ono et al. for single-photon emission computed tomography (SPECT) of Alzheimer’s disease (AD) by targeting β-amyloid (Aβ) (1).

AD is characterized in pathology by the presence of extracellular Aβ plaques, intraneuronal neurofibrillary tangles, and neuronal loss in the cerebral cortex (2, 3). Of them, Aβ deposit is the earliest neuropathological marker and is relatively specific to AD and closely related disorders. Aβ plaques are composed of abnormal paired helical filaments 5–10 nm in size. These filaments are largely made of insoluble Aβ peptides that are 40 or 42 amino acids in length (4).

In recent years, molecular imaging by targeting the extracellular Aβ has been intensively investigated in attempts to detect early AD, assess Aβ content in vivo, determine the timing of anti-plaque therapy, and evaluate the therapeutic efficacy (4). Radiolabeled Aβ40 peptides were tested first, but they showed poor penetration ability to cross the blood–brain barrier (BBB) (4). Based on the fact that Aβ can be specifically stained in vitro with dyes of Congo red, chrysamine G, and thioflavin-T, an effort was made to develop imaging agents with these dyes. This effort, however, was in general unsuccessful because the bulky ionic groups of heteroatoms in these dyes prevent them from crossing the BBB (2). Importantly, a large class of derivatives (e.g., aminonaphthalenes, benzothiazoles, stilbenes, and imidazopyridines) was synthesized with these dyes as templates (4). Clinical and preclinical studies have shown that these derivatives not only possess a high binding affinity with Aβ plaques as their parent compounds, but also exhibit good penetration ability through the BBB and rapid washout from brain with low to no plaque deposits.

Ono et al. first synthesized a class of radioiodinated flavone derivatives that present a high binding affinity with Aβ plaques and good penetration ability through the BBB (5). However, these flavone derivatives display poor clearance from the brain, which leads to a high brain background. The investigators then explored another class of flavonoids with aurone as the core structure (1, 6). Aurone is a heterocyclic chemical compound that contains a benzofuran element associated with a benzylidene linked in position 2 and a chalcone-like group closed into a five-member ring. The aurone derivatives possess a nucleophilic group (NH_2_, NHMe, or NMe_2_) at the 4' position and a radioiodine at the 5 position. Although these aurone derivatives exhibit a strong binding affinity with Aβ (inhibition constant (K_i_) = 1.2–6.8 nM), high penetration ability through the BBB (1.9%−4.6% injected dose per gram tissue (ID/g) at 2 min), and a fast washout from the brain (0.3%−0.5% ID/g at 30 min), the pharmacokinetics of these compounds are less favorable for brain imaging than the pharmacokinetics of the agent [^123^I]IMPY (6-iodo-2-(4'-dimethylamino)phenyl-imidazo[1,2]pyridine), which is the only SPECT agent to be tested in humans to date (7-9). The investigators also modified the flavone and aurone derivatives by pegylating them with 1–3 units of ethylene glycol at the 4' position or by conjugating them with the chelating agent bis-amino-bis-thiol (BAT). Favorable pharmacokinetics for brain imaging was observed for the pegylated derivatives ([^18^F]8(a–c)) but not for the BAT-chelated derivatives ([^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR) (1, 6).

This series of chapters summarizes the data obtained with flavone and aurone derivatives, including [^125^I]15, [^125^I]9, [^125^I]14, [^125^I]16, [^125^I]17, [^99m^Tc]BAT-FL, [^99m^Tc]BAT-AR, [^18^F]8(a–c), [^125^I]3, and [^18^F]3 (1, 6-8). This chapter presents the data obtained with [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR (1).

### Related Resource Links:

- Amyloid-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amyloid+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Amyloid-targeted imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amyloid)
- Structures and other information of amyloid peptides in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=amyloid)
- Alzheimer’s disease articles in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim/?term=Alzheimer%27s%20disease)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20797860)]

The synthesis of the compound precursors with chemical yields was described in detail by Ono et al. (1). [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR were prepared by a ligand exchange reaction with ^99m^Tc-glucoheptonate. Both agents showed a single radioactive complex with a radiochemical purity of >95% after purification with high-performance liquid chromatography (HPLC). The retention times for [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR with HPLC (radioactivity) were 11.1 and 16.6 min, respectively. The radiochemical yields and specific activities for both agents were not reported. The log P values of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR were 2.77 ± 0.04 and 2.23 ± 0.04, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20797860)]

The binding affinities of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR were measured with Aβ(1−42) aggregates in solutions (1). The percent radioactivity of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR bound to aggregates increased with increased dose of Aβ(1–42), while [^99m^Tc]BAT without the flavone and aurone compounds showed no marked affinity for the aggregates. At all concentrations of Aβ aggregates, [^99m^Tc]BAT-AR showed significantly greater affinity than [^99m^Tc]BAT-FL. The nonspecific binding of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR was estimated at 1.62%–1.85%. The affinities of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR were less than those of ^99m^Tc-labeled chalcone derivatives (e.g., ^99m^Tc-BAT-chalcone or [^99m^Tc]17) (10).

The binding of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR with mouse Aβ plaques was confirmed with fluorescent staining in the brain sections of double transgenic AD mice (Tg2576) (1). Amyloid plaques were clearly stained with compound 3, and the labeling pattern was consistent with that observed with thioflavin S staining. Although [^99m^Tc]BAT-AR showed greater affinity than [^99m^Tc]BAT-AR in the in vitro binding assays, no binding difference was observed between [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR with fluorescent staining.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20797860)]

The biodistribution of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR was studied in normal mice (n = 3–6 mice/time point for each agent) (1). The initial brain uptake values for [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR were 0.64% ID/g and 0.79% ID/g at 2 min, and they decreased to 0.23% ID/g and 0.11% ID/g at 60 min after injection, respectively. Compared with that of the ^99m^Tc-labeled chalcone derivative (^99m^Tc-BAT-chalcone or [^99m^Tc]17), the radioactivity of [^99m^Tc]BAT-FL and [^99m^Tc]BAT-AR in the brain appears insufficient for the imaging of Aβ plaques (1, 10). The results showed that the scaffolds of the [^99m^Tc]BAT complexes did not play an important role in the affinity for Aβ aggregates and in the improvement of the pharmacokinetics of flavone and aurone derivatives.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Ono M., Ikeoka R., Watanabe H., Kimura H., Fuchigami T., Haratake M., Saji H., Nakayama M. (2010). 99mTc/Re complexes based on flavone and aurone as SPECT probes for imaging cerebral beta-amyloid plaques. Bioorg Med Chem Lett.
2 Ono M. (2009). Development of positron-emission tomography/single-photon emission computed tomography imaging probes for in vivo detection of beta-amyloid plaques in Alzheimer's brains. Chem Pharm Bull (Tokyo).
3 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
4 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
5 Ono M., Maya Y., Haratake M., Ito K., Mori H., Nakayama M. (2007). Aurones serve as probes of beta-amyloid plaques in Alzheimer's disease. Biochem Biophys Res Commun.
6 Ono M., Watanabe R., Kawashima H., Kawai T., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). 18F-labeled flavones for in vivo imaging of beta-amyloid plaques in Alzheimer's brains. Bioorg Med Chem.
7 Maya Y., Ono M., Watanabe H., Haratake M., Saji H., Nakayama M. (2009). Novel radioiodinated aurones as probes for SPECT imaging of beta-amyloid plaques in the brain. Bioconjug Chem.
8 Watanabe H., Ono M., Kimura H., Kagawa S., Nishii R., Fuchigami T., Haratake M., Nakayama M., Saji H. (2011). A dual fluorinated and iodinated radiotracer for PET and SPECT imaging of beta-amyloid plaques in the brain. Bioorg Med Chem Lett.
9 Newberg A.B., Wintering N.A., Plossl K., Hochold J., Stabin M.G., Watson M., Skovronsky D., Clark C.M., Kung M.P., Kung H.F. (2006). Safety, biodistribution, and dosimetry of 123I-IMPY: a novel amyloid plaque-imaging agent for the diagnosis of Alzheimer's disease. J Nucl Med.
10 Ono M., Ikeoka R., Watanabe H., Kimura H., Fuchigami T., Haratake M., Saji H., Nakayama M. (2010). Synthesis and evaluation of novel chalcone derivatives with 99mTc/Re complexes as potential probes for detection of β-amyloid plaques. ACS Chemical Neuroscience.